# Microbubbles coated with biotinylated rabbit anti-mouse α_V_β_3_ integrin monoclonal antibody

Chemical name: | Microbubbles coated with rabbit anti-mouse α_V_β_3_ integrin monoclonal antibody
Abbreviated name: | MB_integrin_
Synonym:
Agent Category: | Antibody
Target: | α_V_β_3_ integrin
Target Category: | Receptor
Method of detection: | Ultrasound
Source of signal / contrast: | Microbubbles
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Ultrasound%20microbubbles&cmd=DetailsSearch)]

Angiogenesis, the development of new vasculature from pre-existing blood vessels (for details see Carmeliet and Jain (1)), is essential for the development, maintenance, progression, and metastasis of neoplastic tumors (2). Therefore, angiogenesis is considered to be the hallmark of cancerous tumors, and early detection of this process can facilitate the initiation of treatment and management of the disease (3). Although there are several known pro-angiogenic biomarkers, among these only α_V_β_3_ integrin (4), endoglin (5), and the vascular endothelial growth factor receptor 2 (VEGFR-2) (6) are well characterized and are overexpressed in many cancerous tumors, such as those of the breast, ovaries, and the pancreas (3). The α_V_β_3_ integrins are heterodimeric cell adhesion molecules that can bind several different endogenous ligands such as fibronectin, von Willebrand factor, fibrinogen, etc., and assist with the survival and migration of cancerous cells, which increases the invasive potential of these cells, and promotes angiogenesis in tumors (7). Endoglin (CD105) is a co-receptor of the transforming growth factor beta (TGF-β) and co-modulates different activities, including angiogenesis, of the activated TGF-β receptor (8). The VEGFR-2 mediates its effects through a family of receptor tyrosine kinases that promote the mitogenesis, survival, differentiation, migration, and vascular permeability of endothelial cells (9).

Little information is available regarding the expression of the different angiogenic markers during the progression of a tumor from a small size to a larger size. Noninvasive visualization of angiogenic markers that are overexpressed during initial stages of the neoplasia can facilitate early detection and treatment of the disease (3). For this, Deshpande et al. developed a series of microbubble (MB; perfluorocarbon gas enclosed within spherical lipid shells harboring streptavidin moieties to bind biotinylated monoclonal antibodies (mAb) directed toward specific targets) based contrast agents that were coated with specific antibodies targeted to α_V_β_3_ integrin (MB_integrin_), endoglin (MB_endoglin_), and VEGFR 2 (MB_vegfr2_), respectively (3). The targeted MBs were then used with ultrasound imaging to determine the expression of the angiogenic biomarkers during the growth of human ovarian (SKOV3 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-77&Template=cellBiology)), human breast (MDA-MB-361 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-27&Template=cellBiology)), and human pancreatic (MiaPaCa2 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1420&Template=cellBiology)) cell line xenograft tumors in mice. This chapter describes the studies performed with MB_integrin_. Studies performed with MB_endoglin_ and MB_vegfr2_ are described in separate chapters of MICAD (www.micad.nih.gov) (10, 11).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Integrin+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Homo sapiens integrin, alpha V, transcript variant 1, protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_002210.3)

Rat (Rattus norvegicus) integrin, beta 3, protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_153720.1)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Integrin) related to integrins

Integrin alpha V in Online Mendelian Inheritance in Man Database (OMIM) (http://omim.org/entry/193210)

Integrin beta 3 in Online Mendelian Inheritance in Man Database (OMIM) (http://omim.org/clinicalSynopsis/173470?search=alpha%20v%20integrin&highlight=alpha%20integrin%20v)

Integrin signaling pathway (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=100123&pathway_name=integrin%20signaling%20pathway&source=BioCarta%20Imported&what=graphic&jpg=on&ppage=1) in Pathway Interaction Database

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis of MB_integrin_ has been described in detail by Deshpande et al. (3). Briefly, the MBs were obtained as a freeze-dried preparation from a commercial source and reconstituted in 1 mL sterile 0.9% sodium chloride. Subsequently, 5 × 10^7^ of the reconstituted MBs were incubated with 5 μg biotinylated anti-mouse α_V_β_3_ integrin mAb for 10 min at room temperature to obtain MB_integrin_. A similar procedure was used to obtain MB_endoglin_ and MB_vegfr2_. For use as controls, another batch of MBs was linked to biotinylated rabbit immunoglobulin G antibodies (MB_control_). The procedure used to remove excess mAb, if any, from the final preparations was not reported. The average number of antibody molecules bound per square micrometer of the MBs of each preparation was reported to be ~7,600 as determined with fluorescence-activated cell sorter analysis (3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MB%20endoglin%20in%20vitro%20studies&cmd=DetailsSearchhttp://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

A parallel plate flow chamber cell-binding assay with SVR cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2280&Template=cellBiology) (the high expression of α_V_β_3_ integrins and the other angiogenic biomarkers by these cells was confirmed with immunofluorescence staining) revealed that, compared to MB_control_, a significantly higher (P = 0.003) amount of MB_integrin_ bound to these cells (3). Little or no binding of these MBs was observed with control cells (4T1 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2539&Template=cellBiology)) that did not express any of the angiogenic biomarkers. An overall significantly positive correlation (ρ = 0.87; P = 0.019) was observed between the number of MBs that attached to the SVR cells and the expression of α_V_β_3_ integrins by the cells. Pre-incubation of the SVR cells with the rabbit anti-mouse α_V_β_3_ integrin mAb was reported to block the binding of MB_integrin_.

An ex vivo immunofluorescence study of the tumor sections showed that α_V_β_3_ integrins in the cells was colocalized with CD31, a biomarker specific for endothelial cells (3). This indicated that the in vivo ultrasound signal obtained from the cancerous lesions was indeed generated by the MB_integrin_ bound to the α_V_β_3_ integrin receptors expressed by the cells in the tumors. In addition, a good correlation (ρ = 0.65) was evident between the in vivo ultrasound imaging signal and the ex vivo expression level of α_V_β_3_ integrins in the tumors (P = 0.05) (3).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MB%20endoglin%20rodentia&cmd=DetailsSearch)]

The expression of α_V_β_3_ integrins was investigated using MB_integrin_ with ultrasound imaging during the different growth stages based on tumor size (small, 50–150 mm^3^; medium, 150–250 mm^3^; large, >250 mm^3^) of subcutaneous breast, ovarian, and pancreatic cell line xenograft tumors in mice (n = 3 animals/tumor type) as described by Deshpande at al (3). In addition, the expression of α_V_β_3_ integrin was compared with that of endoglin and VEGFR-2 in these lesions.

Using the different MB based mAbs, ultrasound visualization of small and medium-sized breast cell line xenograft tumors in mice showed that the lesions expressed approximately the same levels (P = 0.70) of α_V_β_3_ integrin and VEGFR-2, but the expression of endoglin in the neoplasm was significantly higher (P ≤ 0.04) than that of α_V_β_3_ integrin and VEGFR-2 (3). A similar level of all the three angiogenic markers was observed in large tumors of the breast cell line (P ≥ 0.08).

Ultrasound imaging with the different MB-antibody preparations showed that the expression of both α_V_β_3_ integrin and VEGFR-2 was lower than that of endoglin (P ≤ 0.04) in all sizes of the ovarian cell line xenograft tumors (3). No significant difference (P ≥ 0.40) was observed in the expression level of α_V_β_3_ integrin and VEGFR-2 in the different sizes of the ovarian cell line lesions.

The small pancreatic cell line xenograft tumors were shown to express higher levels of α_V_β_3_ integrin compared with either endoglin (P = 0.15) or VEGFR-2 (P = 0.07) (3). No significant difference in the expression level of the three angiogenic markers in the medium-sized pancreatic cell line tumors was observed. The large pancreatic lesions showed a significantly higher (P = 0.01) expression of endoglin compared with VEGFR2 (P = 0.22).

From these studies, the investigators concluded that the expression level of the different angiogenic markers varies with the growth stage of the tumor (3). They also concluded that targeted MB-based contrast agents can be used with ultrasound imaging to detect tumors in the early stages of growth in mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MB%20endoglin%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MB%20endoglin%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MB%20endoglin%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No Supplemental Information is currently available.

## References

1 Carmeliet P., Jain R.K. (2011). Molecular mechanisms and clinical applications of angiogenesis. Nature.
2 De Bock K., Mazzone M., Carmeliet P. (2011). Antiangiogenic therapy, hypoxia, and metastasis: risky liaisons, or not?. Nat Rev Clin Oncol.
3 Deshpande N., Ren Y., Foygel K., Rosenberg J., Willmann J.K. (2011). Tumor angiogenic marker expression levels during tumor growth: longitudinal assessment with molecularly targeted microbubbles and US imaging. Radiology.
4 Cai W., Chen X. (2006). Anti-angiogenic cancer therapy based on integrin alphavbeta3 antagonism. Anticancer Agents Med Chem.
5 Nassiri F., Cusimano M.D., Scheithauer B.W., Rotondo F., Fazio A., Yousef G.M., Syro L.V., Kovacs K., Lloyd R.V. (2011). Endoglin (CD105): a review of its role in angiogenesis and tumor diagnosis, progression and therapy. Anticancer Res.
6 Shibuya M., Claesson-Welsh L. (2006). Signal transduction by VEGF receptors in regulation of angiogenesis and lymphangiogenesis. Exp Cell Res.
7 Wu G., Wang X., Deng G., Wu L., Ju S., Teng G., Yao Y., Liu N. (2011). Novel peptide targeting integrin alphavbeta3-rich tumor cells by magnetic resonance imaging. J Magn Reson Imaging.
8 Perez-Gomez E., Del Castillo G., Juan Francisco S., Lopez-Novoa J.M., Bernabeu C., Quintanilla M. (2010). The role of the TGF-beta coreceptor endoglin in cancer. ScientificWorldJournal.
9 Koch S., Tugues S., Li X., Gualandi L., Claesson-Welsh L. (2011). Signal transduction by vascular endothelial growth factor receptors. Biochem J.
10 Chopra, A., Microbubbles coated with biotinylated rabbit anti-mouse endoglin monoclonal antibody. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
11 Chopra, A., Microbubbles coated with biotinylated rabbit anti-mouse vascular endothelial growth factor receptor 2 monoclonal antibody. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.